# ^68^Ga-1,4,7-Triazacyclononane-1,4-7-triacetic acid-Glu-[15-amino-4,7,10,13-tetraoxapentadecanoic acid-c(Arg-Gly-Asp-D-Phe-Lys)]_2_

Chemical name: | ^68^Ga-1,4,7-Triazacyclononane-1,4-7-triacetic acid-Glu-[15-amino-4,7,10,13-tetraoxapentadecanoic acid-c(Arg-Gly-Asp-D-Phe-Lys)]_2_
Abbreviated name: | ^68^Ga-NOTA-P_4_-RGD2, ^68^Ga-NOTA-E-[PEG_4_-c(RGDfK)]_2_
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. The α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). The peptide sequence Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most of the cyclic RGD peptides are composed of five amino acids. Various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (50% inhibition concentration (IC_50_), 7–40 nM) but not to α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM) integrins (11). Various radiolabeled cyclic RGD peptides and peptidominetics have been found to have high accumulation in tumors in mice (12, 13). Out of these developments [^18^F]Galacto-c(RGDfK) has been evaluated in a number of clinical studies for imaging of α_v_β_3_ in cancer patients (14-19). Liu et al. (20) used 1,4,7-triazacyclononane-1,4-7-triacetic acid (NOTA) as a bifunctional chelator for labeling Glu-[15-amino-4,7,10,13-tetraoxapentadecanoic acid-cyclo(RGDfK)]_2_ (P_4_-RGD2) to form (^68^Ga-NOTA-P_4_-RGD2) for positron emission tomography (PET) imaging of α_v_β_3_ receptors in nude mice bearing human glioblastoma U87MG tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+synthesis)]

P_4_-RGD2 was prepared with solid-phase peptide synthesis (20). Addition of the NOTA group to P_4_-RGD2 was performed by mixing 2 µmol P_4_-RGD2 with 6 μmol S-2-(4-isothiocyanatobenzyl)-NOTA in sodium bicarbonate buffer (pH 9) for 5 h at room temperature. NOTA-P_4_-RGD2 was isolated with high-performance liquid chromatography (HPLC) with 42% yield and >95% purity. Molecular weight was determined with MALDI-TOF-MS to be m/z 2,265.80 Da (calculated molecular weight, 2,263.52 Da). For ^68^Ga labeling, a solution of 185 MBq (5 mCi) ^68^GaCl_3_ and 10 nmol RGD2 was heated for 10 min at 42°C. ^68^Ga-NOTA-P_4_-RGD2 was purified with HPLC with a yield of 92% and a radiochemical purity of >98%. The specific activity was 9.8–11.8 MBq/nmol (0.26–0.32 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+in+vitro)]

Liu et al. (20) performed in vitro inhibition studies of NOTA-P_4_-RGD2 in cultured human U87MG cells with ^125^I-echistatin. The IC_50_ values were 88.8, 41.8, 100.0, and 34.0 nM for RGD2, P_4_-RGD2, NOTA-RGD2, and NOTA-P_4_-RGD2, respectively. These comparable IC_50_ values indicated that NOTA and P_4_ conjugation had little effect on the receptor binding affinity.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+%20rodentia)]

Liu et al. (20) performed ex vivo biodistribution studies of 0.37 MBq (10 μCi) ^68^Ga-NOTA-P_4_-RGD2 or ^68^Ga-NOTA-RGD2 in nude mice bearing U87MG xenografts at 1 h after injection. Tumor accumulation was 7.98 ± 0.94% and 4.17 ± 1.10% injected dose per gram (ID/g) for ^68^Ga-NOTA-P_4_-RGD2 and ^68^Ga-NOTA-RGD2, respectively. The tumor/muscle ratios were 6.4 and 2.9 for ^68^Ga-NOTA-P_4_-RGD2 and ^68^Ga-NOTA-RGD2, respectively. Therefore, the P_4_-linkers improved the tumor accumulation. The kidney accumulation was 11.6% ID/g for ^68^Ga-NOTA-P_4_-RGD2 and 11.1% ID/g for ^68^Ga-NOTA-RGD2. Coinjection of excess c(RGDyK) (10 mg/kg) and ^68^Ga-NOTA-RGD2 inhibited the tumor accumulation by 80%, whereas the accumulation in the kidneys was inhibited by only 30%. Various small inhibitory effects were also observed in the other tissues and organs. Quantitative analyses of PET imaging data showed that the radioactivity levels in the U87MG tumors (n = 4 mice) were 10.13 ± 1.81% ID/g (30 min), 7.40 ± 0.39% ID/g (60 min), and 7.24 ± 0.45% ID/g (120 min) for ^68^Ga-NOTA-P_4_-RGD2. ^68^Ga-NOTA-P_4_-RGD2 was excreted mainly through the kidneys. Coinjection of c(RGDyK) and ^68^Ga-NOTA-P_4_-RGD2 reduced the tumor accumulation to the background level with 81% inhibition at 60 min after injection. The tumor/muscle, tumor/liver, tumor/blood, and tumor/kidney ratios for ^68^Ga-NOTA-P_4_-RGD2 were significantly higher than those for ^68^Ga-NOTA-RGD2 (P < 0.01) at the three time points.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+NOTA+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Haubner R., Decristoforo C. (2009). Radiolabelled RGD peptides and peptidomimetics for tumour targeting. Front Biosci.
13 Schottelius M., Laufer B., Kessler H., Wester H.J. (2009). Ligands for mapping alphavbeta3-integrin expression in vivo. Acc Chem Res.
14 Beer A.J., Grosu A.L., Carlsen J., Kolk A., Sarbia M., Stangier I., Watzlowik P., Wester H.J., Haubner R., Schwaiger M. (2007). [18F]galacto-RGD positron emission tomography for imaging of alphavbeta3 expression on the neovasculature in patients with squamous cell carcinoma of the head and neck. Clin Cancer Res.
15 Beer A.J., Haubner R., Goebel M., Luderschmidt S., Spilker M.E., Wester H.J., Weber W.A., Schwaiger M. (2005). Biodistribution and pharmacokinetics of the alphavbeta3-selective tracer 18F-galacto-RGD in cancer patients. J Nucl Med.
16 Beer A.J., Haubner R., Sarbia M., Goebel M., Luderschmidt S., Grosu A.L., Schnell O., Niemeyer M., Kessler H., Wester H.J., Weber W.A., Schwaiger M. (2006). Positron emission tomography using [18F]Galacto-RGD identifies the level of integrin alpha(v)beta3 expression in man. Clin Cancer Res.
17 Beer A.J., Lorenzen S., Metz S., Herrmann K., Watzlowik P., Wester H.J., Peschel C., Lordick F., Schwaiger M. (2008). Comparison of integrin alphaVbeta3 expression and glucose metabolism in primary and metastatic lesions in cancer patients: a PET study using 18F-galacto-RGD and 18F-FDG. J Nucl Med.
18 Beer A.J., Niemeyer M., Carlsen J., Sarbia M., Nahrig J., Watzlowik P., Wester H.J., Harbeck N., Schwaiger M. (2008). Patterns of alphavbeta3 expression in primary and metastatic human breast cancer as shown by 18F-Galacto-RGD PET. J Nucl Med.
19 Haubner R., Weber W.A., Beer A.J., Vabuliene E., Reim D., Sarbia M., Becker K.F., Goebel M., Hein R., Wester H.J., Kessler H., Schwaiger M. (2005). Noninvasive visualization of the activated alphavbeta3 integrin in cancer patients by positron emission tomography and [18F]Galacto-RGD. PLoS Med.
20 Liu Z., Niu G., Shi J., Liu S., Wang F., Liu S., Chen X. (2009). (68)Ga-labeled cyclic RGD dimers with Gly3 and PEG4 linkers: promising agents for tumor integrin alphavbeta3 PET imaging. Eur J Nucl Med Mol Imaging.